# 1-(2-[^18^F]Fluoro-3-pyridyl)-4-(2-isopropyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole

Chemical name: | 1-(2-[^18^F]Fluoro-3-pyridyl)-4-(2-isopropyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole
Abbreviated name: | [^18^F]FPIT
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FPIT)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, with low density in the cerebellum. mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting mGluR1 can visualize and analyze mGluR1 expression in normal physiological and pathological conditions. Several radioligands have been studied for in vivo imaging of mGluR1 in the brain. 1-(2-Fluoro-3-pyridyl)-4-(2-isopropyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole (FPIT) was shown to be a selective mGluR1 with nanomolar affinity (5.4 nM) with little inhibition to mGluR5 (5). Fujinaga et al. (6) prepared and evaluated 1-(2-[^18^F]Fluoro-3-pyridyl)-4-(2-isopropyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole ([^18^F]FPIT) for use with in vivo PET imaging of mGluR1 distribution in the brain with small animals and monkeys.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20synthesis)]

Fujinaga et al. (6) reported an one-step automated synthesis of [^18^F]FPIT. The bromo-precursor was subjected to nucleophilic fluorination with K[^18^F]F for 10 min at 150°C, with a radiochemical yield of 58 ± 21% (n = 16) and a specific activity of 80–280 GBq/μmol (2.2–7.6 Ci/μmol) after purification with high-performance liquid chromatography. The radiochemical purity of [^18^F]FPIT was >98%. The total synthesis time was 77 min. [^18^F]FPIT exhibited a Log D_7.4_ value of 2.53 ± 0.19 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20in%20vitro)]

In vitro [^18^F]FPIT autoradiographic imaging studies were performed on rat brain sections (n = 8/group) (6). [^18^F]FPIT bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum (333 ± 47 PSL/mm^2^) and thalamus (237 ± 35 PSL/mm^2^), followed by the hippocampus (158 ± 30 PSL/mm^2^), striatum (98 ± 27 PSL/mm^2^), cerebral cortex (49 ± 10 PSL/mm^2^) and pons-medulla (26 ± 5 PSL/mm^2^). FPIT and JNJ-16259685 (1,000 nM, mGluR1 antagonists) completely blocked radioactive signals to background levels in these brain regions. On the other hand, mGluR5 antagonist MPEP (1,000 nM) only demonstrated only marginal inhibition of the signals. In vitro autoradiographic studies were also performed on monkey brain sections (n = 10/group) with similar results as those of the rat brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20rodentia)]

Fujinaga et al. (6) performed ex vivo biodistribution studies in rats (n = 4/group) at 1-90 min after intravenous injections of 3.4 MBq (0.46 mCi) [^18^F]FPIT (0.014 nmol). The radioactivity levels in most tissues were highest at 1-5 min and thereafter decreased quickly. The highest accumulation at 5 min was observed in the liver (2.07% injected dose/gram (ID/g)), followed by the small intestine (1.64% ID/g), kidney (1.55% ID/g), lung (1.54% ID/g), pancreas (1.28% ID/g), brain (0.98% ID/g), spleen (0.95% ID/g), heart (0.61% ID/g), muscle (0.33% ID/g), blood (0.32% ID/g), and bone (0.39% ID/g). [^18^F]FPIT remained 42% and 93% intact in the plasma and brain at 60 min, respectively.

Fujinaga et al. (6) performed dynamic PET imaging studies for 90 min in rats (n = 4/group) after intravenous injection of 19 MBq (0.51 mCi) [^18^F]FPIT (0.08 nmol). Blocking studies were performed by pretreatment (0.5 min) with 1 mg/kg FPIT, JNJ-16259685 or MPEP. Baseline tissue time-activity curves revealed a high accumulation of radioactivity peaked at 30 min in the cerebellum, and decreased to 87% of the maximum at 90 min. On the other hand, moderate radioactivity levels in the thalamus, striatum, hippocampus and cerebral cortex peaked at 5-10 min and decreased to 60-70% of the maximum at 90 min. The cerebellum/medulla, thalamus/medulla, striatum/medulla, hippocampus/medulla, and cerebral cortex/medulla ratios at 10-15 min were 4.27, 2.32, 1.82, 1.61, and 1.42, respectively. The non-displacement binding potential (BP_nd_) values were 2.10 ± 0.18 and 0.60 ± 0.04 for the cerebellum and thalamus as determined with the simplified reference-tissue model, respectively. Pretreatment with FPIT reduced the radioactivity signals by 83%, 71%, 62%, 61% and 53% in the cerebellum, thalamus, striatum, hippocampus, and cerebral cortex, respectively. Pretreatment with JNJ-16259685 also showed reduced radioactivity levels in all brain regions, whereas pretreatment with MPEP showed little inhibition.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20%28primate%20not%20human%29)]

Fujinaga et al. (6) performed dynamic PET imaging studies for 90 min in one male rhesus monkey after intravenous injection of 152 MBq (4.1 mCi, 0.63 nmol) [^18^F]FPIT. Blocking studies were performed by pretreatment (0.5 min) with FPIT (1 mg/kg), JNJ-16259685 (3 mg/kg) or MPEP (1 mg/kg). Baseline tissue time-activity curves revealed high accumulation of radioactivity in the cerebellum, followed by the thalamus. However, little difference in radioactivity levels was observed among the striatum, hippocampus, cingulate cortex, and pons. The maximum uptake ratios to the pons were 1.62, 1.43 and 1.00-1.25 for the cerebellum, thalamus, and the rest of brain regions, respectively. Pretreatment with JNJ-16259685 or FPIT reduced the radioactivity signals of all brain regions by 40-70%, whereas pretreatment with MPEP did no change the distribution of radioactivity in the brain. [^18^F]FPIT remained 89% and 50% intact in the brain and plasma at 90 min, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPIT%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Hostetler E.D., Eng W., Joshi A.D., Sanabria-Bohorquez S., Kawamoto H., Ito S., O'Malley S., Krause S., Ryan C., Patel S., Williams M., Riffel K., Suzuki G., Ozaki S., Ohta H., Cook J., Burns H.D., Hargreaves R. (2011). Synthesis, characterization, and monkey PET studies of [(1)(8)F]MK-1312, a PET tracer for quantification of mGluR1 receptor occupancy by MK-5435. Synapse.
6 Fujinaga M., Maeda J., Yui J., Hatori A., Yamasaki T., Kawamura K., Kumata K., Yoshida Y., Nagai Y., Higuchi M., Suhara T., Fukumura T., Zhang M.R. (2012). Characterization of 1-(2-[18F] fluoro-3-pyridyl)-4-(2-isopropyl-1-oxo- isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole, a PET ligand for imaging the metabotropic glutamate receptor type 1 in rat and monkey brains. J Neurochem.